# ^177^Lu-Labeled aglycosylated anti-L1-CAM monoclonal antibody chCE7

Chemical name: | ^177^Lu-Labeled aglycosylated anti-L1-CAM monoclonal antibody chCE7
Abbreviated name: | [^177^Lu]-chCE7agl
Synonym:
Agent Category: | Antibody
Target: | L1-CAM antigen
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=chCE7agl&cmd=DetailsSearch)]

Expression of the L1-cell adhesion molecule (L1-CAM) is reported to correlate with and is required for the progression and metastasis of many cancers, including that of the ovaries (1). Therefore, the L1-CAM has been targeted for the therapy of many cancers, as discussed in detail by Weidle et al. (2). The chimeric monoclonal antibody (mAb) chCE7, directed toward the L1-CAM, has been shown to have a very high affinity for the antigen (K_d_ ~1 pmol/L) and to inhibit the proliferation of ovarian cancer cells in vitro (3). However, in a preliminary clinical study it was shown that, although the ^131^I-labeled mAb was suitable for the imaging of rapidly growing cancerous lesions in patients, it could not detect the large metastasized tumors in the individuals (4). In another study, ^177^Lu- and ^67/64^Cu-labeled F(ab')_2_ fragments of chCE7 were evaluated in nude mice for radioimmunotherapy (RIT) and positron emission tomographic imaging of intraperitoneal (i.p.) SKOV3 cell (SKOV3ip; of human ovarian cancer origin) tumors that express the L1-CAM antigen (5). Although the ^177^Lu- and the ^67/64^Cu-labeled fragments of the mAb were able to detect the tumors at 24 h postinjection (p.i.), a very high proportion of radioactivity from both radiolabeled mAbs (34.5% of total injected dose per gram tissue (% ID/g) and 16.0% ID/g for ^177^Lu and ^67^Cu, respectively) was observed to accumulate in the kidneys of the animals (5). From these studies, the investigators concluded that a radiolabeled variant of the chCE7 that can clear rapidly from circulation and show low accumulation of radioactivity in the kidneys will have to be developed for the RIT of cancerous tumors that overexpress the L1-CAM antigen. To circumvent these problems, an aglycosylated form of chCE7 was engineered (chCE7agl) by substituting the asparagine residue at position 297 (a glycosylation site) with glutamine in the heavy chain of the mAb (3). A biodistribution study of ^67^Cu-labeled chCE7agl in nude mice bearing SKOV3ip tumors showed that there was a high and persistent uptake of radioactivity in the lesions and that a single dose of [^67^Cu]-chCE7agl reduced the growth of the tumor and prolonged the survival of the rodents (3). This study suggested that aglycosylation of chCE7 improved the pharmacokinetics, biodistribution, and therapeutic efficacy of the mAb.

To enhance the RIT efficacy of a mAb, it is important to label it with a radionuclide that is readily available, has a reasonable half-life, and emits medium-energy β-particles (6). The metallic radionuclide ^177^Lu falls into this category (half-life, 6.7 days; mean range, 0.2 mm; %B = 100) and has been used widely to label mAbs and peptides for imaging and RIT studies in animals and humans [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu&cmd=DetailsSearch)]. The chCE7agl mAb was labeled with ^177^Lu ([^177^Lu]-chCE7agl), and the in vitro and in vivo properties of the labeled mAb, including biodistribution, were investigated in normal nude mice or nude mice bearing SKOV3ip tumors (1, 6).

### Related Resource Links

Chapters related to CAMs in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Cell+adhesion+molecule+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Cell+adhesion+molecule) related to CAMs

Human L1-CAM protein and mRNA (variant 3) sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_001143963.1)

L1-CAM (http://omim.org/entry/308840) in Online Mendelian Inheritance in Man Database (OMIM)

Information on L1-CAM in Kyoto Encyclopedia of Genes and Genomics (KEGG) (http://www.genome.jp/dbget-bin/www_bget?hsa:3897)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-chCE7agl%20synthesis&cmd=DetailsSearch)]

The chCE7agl mAb was produced in and purified from HEK-293 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1573&Template=cellBiology) cells as described elsewhere (6). The mAb was conjugated to 1,4,7,10-tetraazacyclododecane-N-N'-N''-N'''-tetraacetic acid (DOTA) for labeling with ^177^Lu, and the number of chelator molecules attached to each molecule of chCE7agl was determined with a spectrometric method as described by Knogler et al. (6). The chelator/mAb ratios of the three DOTA-chCE7agi conjugates were determined to be 7, 12, and 15, respectively, and were dependent on the molar excess ratio of DOTA (with respect to chCE7agl) used in the coupling reaction (6). After labeling with ^177^Lu, the specific activities of chCE7agl conjugated to 7, 12, or 15 groups of DOTA were 30 MBq/6.66 nmol (0.8 mCi/6.66 nmol), 106 MBq/6.66 nmol (2.82 mCi/6.66 nmol), and 103 MBq/6.66 nmol (2.78 mCi/6.66 nmol), respectively. The radiochemical yields of the labeled mAbs ranged from 4.5% to 59.0%. The radiochemical purity (RCP) of the final product was not reported.

In another publication, an average of 4.2 DOTA molecules were reported to be conjugated with each molecule of chCE7agl (1). After labeling with ^177^Lu, the immunoconjugate had a specific activity ranging from 52–153 MBq/6.66 nmol (1.4–4.1 Ci/6.66 nmol), and the labeling efficiency of the reaction was between 62% and 87%. The RCP and the stability of the labeled mAb were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-chCE7agl%20in%20vitro&cmd=DetailsSearch)]

The stability of the immunoconjugate containing 12 chelator molecules was determined by incubating 1 pmol [^177^Lu]-chCE7agl in 1 ml human plasma for 24 h at 37°C (6). The labeled mAb remained stable under these experimental conditions (no release of ^177^Lu or denaturation of the complex) as determined with high-performance liquid chromatographic analysis and size-exclusion chromatography (6).

In a competition assay with ^125^I-labeled chCE7agl as the ligand and SKVO3ip cells as the target, the IC_50_ values of chCE7agl conjugated to 7, 12, or 15 DOTA molecules were determined to be 0.79 pmol, 1.36 pmol, and 6.58 pmol, respectively (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-chCE7agl%20rodentia&cmd=DetailsSearch)]

Knogler et al. investigated the biodistribution of [^177^Lu]-chCE7agl coupled to different numbers of DOTA groups in the blood and liver of normal nude mice (Table 1) (6). The rodents (n = 3 mice/group) were injected with ~0.3 MBq (8.1 μCi) of the labeled conjugates through the tail vein, and the animals were euthanized at either 24 h p.i. (for immunoconjugates with 12 or 15 DOTA) or at 48 h p.i. (for the immunocomplex with 7 DOTA). Subsequently, the blood and liver of the mice were collected to determine the amount of radioactivity accumulated in these tissues.

Table 1: Accumulation of radioactivity with different DOTA-chCE7agl conjugates in the blood and liver of normal nude mice ( 6 ).

DOTA/chCE7agl ratio | Accumulated radioactivity (% ID/g) | | Liver/Blood ratio | Time p.i. (h)
DOTA/chCE7agl ratio | Blood | Liver | Liver/Blood ratio | Time p.i. (h)
7 | 12.03 ± 2.22 | 3.99 ± 1.10 | 0.33 | 48
12 | 12.16 ± 4.13 | 14.67 ± 8.88 | 1.20 | 24
15 | 1.81 ± 0.36 | 30.96 ± 0.79 | 17.10 | 24

From Table 1 it is clear that the DOTA/mAb ratio influenced the liver/blood ratio of the immunoconjugates. Among the different DOTA-chCE7agl conjugates, only conjugates with 7 and 12 DOTA molecules showed slow clearance from the blood and had a low accumulation in the liver. The conjugate with 15 DOTA coupled to the mAb exhibited rapid clearance from blood and had a very high accumulation in the liver (liver/blood ratio = 17.10).

Fischer et al. investigated the biodistribution of [^177^Lu]-chCE7agl in CD1-Foxn^nu^ mice bearing intraperitoneal SKOV3ip1 tumors (1). The animals (n = at least 4 mice/time point) were injected with 4 MBq (~110 μCi; ~200 pmol) labeled mAb through the tail vein and euthanized at time points ranging from 24 h p.i. (1 d p.i.) to 336 h p.i. (14 d p.i.). All the organs of interest, including blood, were harvested from the rodents to quantify the accumulation of radioactivity in the various tissues. At 24 h p.i., the amount of tracer in the blood, liver, and tumors was 12.5 ± 2.5% ID/g, 6.5 ± 1.8% ID/g, and 29.1 ± 6.3% ID/g, respectively. The peak accumulation of label in the tumors was 48.0 ± 8.1% ID/g at 168 h p.i. (7 d p.i.), and the amount of radioactivity in the blood and liver at this time point was 2.2 ± 0.8% ID/g and 3.1 ± 0.2% ID/g, respectively. At 168 h p.i., all other organs had an accumulation of <3.5 ± 1.2% ID/g (spleen) of the tracer. A high level of the label was present in the tumors even at 336 h p.i. (22.8 ± 5.2% ID/g), whereas all other organs, except the spleen, showed an accumulation of <2.1 ± 0.07% ID/g in the tissues. The uptake of radioactivity in the spleen was 6.4 ± 1.0% ID/g at this time point. No blocking studies were reported.

For single-photon emission computed tomographic (SPECT) and computed tomographic (CT) imaging, CD1-Foxn^nu^ mice (the number of animals was not reported) bearing either subcutaneous (s.c.; located on the shoulders) or SKOV3ip1 cell tumors were injected with [^177^Lu]-chCE7agl through a lateral tail vein (1). Mice without tumors served as controls and were injected with a similar amount of radioactivity through the same route as the test animals. SPECT/CT images acquired from the animals at 48 h p.i. showed that the s.c and the i.p. tumors accumulated a high amount of the tracer and were clearly visible in the animals. In addition, disseminated tumor nodules were also visible in animals with the i.p. tumors. No radioactivity was evident in the blood pool or other organs of the control mice or animals bearing the s.c. or i.p. tumors. No blocking studies were reported to determine saturable binding.

From these studies, the investigators concluded that [^177^Lu]-chCE7agl can be used for the RIT of tumors that overexpress the L1-CAM antigen in rodents (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-chCE7agl%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-chCE7agl%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-chCE7agl%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Fischer E., Grunberg J., Cohrs S., Hohn A., Waldner-Knogler K., Jeger S., Zimmermann K., Novak-Hofer I., Schibli R. (2012). L1-CAM-targeted antibody therapy and (177)Lu-radioimmunotherapy of disseminated ovarian cancer. Int J Cancer.
2 Weidle U.H., Eggle D., Klostermann S. (2009). L1-CAM as a target for treatment of cancer with monoclonal antibodies. Anticancer Res.
3 Knogler K., Grunberg J., Zimmermann K., Cohrs S., Honer M., Ametamey S., Altevogt P., Fogel M., Schubiger P.A., Novak-Hofer I. (2007). Copper-67 radioimmunotherapy and growth inhibition by anti-L1-cell adhesion molecule monoclonal antibodies in a therapy model of ovarian cancer metastasis. Clin Cancer Res.
4 Hoefnagel C.A., Rutgers M., Buitenhuis C.K., Smets L.A., de Kraker J., Meli M., Carrel F., Amstutz H., Schubiger P.A., Novak-Hofer I. (2001). A comparison of targeting of neuroblastoma with mIBG and anti L1-CAM antibody mAb chCE7: therapeutic efficacy in a neuroblastoma xenograft model and imaging of neuroblastoma patients. Eur J Nucl Med.
5 Grunberg J., Novak-Hofer I., Honer M., Zimmermann K., Knogler K., Blauenstein P., Ametamey S., Maecke H.R., Schubiger P.A. (2005). In vivo evaluation of 177Lu- and 67/64Cu-labeled recombinant fragments of antibody chCE7 for radioimmunotherapy and PET imaging of L1-CAM-positive tumors. Clin Cancer Res.
6 Knogler K., Grunberg J., Novak-Hofer I., Zimmermann K., Schubiger P.A. (2006). Evaluation of 177Lu-DOTA-labeled aglycosylated monoclonal anti-L1-CAM antibody chCE7: influence of the number of chelators on the in vitro and in vivo properties. Nucl Med Biol.